# ^64^Cu-1,4,7,10-Tetraazacyclododecane-1,4,7,10-tetraacetic acid-anti-CD105 TRC105 chimeric monoclonal antibody

Chemical name: | ^64^Cu-1,4,7,10-Tetraazacyclododecane-1,4,7,10-tetraacetic acid-anti-CD105 TRC105 chimeric monoclonal antibody
Abbreviated name: | ^64^Cu-DOTA-TRC105
Synonym:
Agent category: | Antibody
Target: | CD105 (Endoglin, EDG)
Target category: | Antigen
Method of detection: | Positron emission tomography (PET)
Source of signal/ contrast: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=4557555), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=10862690) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=2022) for more information about CD105

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=TRC105)]

Angiogenesis is an essential process in the development of new blood vessels both in normal physiological states and diseases (1, 2). Targeting of tumor vasculature is a promising strategy for tumor imaging and therapy because tumor growth and metastasis largely depend on angiogenesis (3-5). Transforming growth factor-β (TGF-β) is a pleiotropic cytokine that modulates blood vessel development, angiogenesis, and tumor progression (6). There are three isoforms of TGF-β (β_1_, β_2_, and β_3_). TGF-β_1_ inhibits proliferation and migration of endothelial cells and their ability to form capillaries. CD105 (endoglin, EDG) is a homodimeric transmembrane glycoprotein (180 kDa) with disulfide-linked subunits of 95 kDa. CD105 is a component of the TGF-β receptor complex that specifically binds TGF-β_1_ and TGF-β_3_ with high affinity (7). CD105 is important for blood vessel development. The expression of CD105 on different cells affects cellular response to TGF-β_1_. CD105 is overexpressed in proliferating endothelial cells of tumor vessels, and CD105 prevents TGF-β_1_-mediated inhibition of endothelial cell proliferation (8, 9).

Radiolabeled monoclonal antibodies (mAbs) have been developed for both the diagnosis and treatment of tumors (10-12). Quiescent human endothelial cells express CD105 only weakly, but the expression of CD105 is strongly upregulated on the endothelium of tumor tissues undergoing angiogenesis (9, 13). The high level of expressed CD105 (up to 10^6^ molecules/proliferating cell) appears to be ideal for in vivo imaging and therapy. Anti-CD105 mAbs, such as MAEND3, E9, and MJ7/18 with radionuclides (e.g., ^111^In, ^99m^Tc, and ^125^I) have been studied as single-photon emission computed tomography (SPECT) probes for imaging CD105 expression (9, 14). TRC105 is a human/murine chimeric IgG_1_ mAb that bind with higher affinity to human CD105 than to murine CD105 (15). TRC105 inhibits angiogenesis and tumor growth and is now in clinical trials in cancer patients. Hong et al. (16) showed that ^64^Cu-1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid-anti-CD105 TRC105 (^64^Cu-DOTA-TRC105) mAbs could efficiently image 4T1 murine breast tumor in mice with positron emission tomography (PET) imaging.

### Related Resource Links:

- Chapters in MICAD (CD105 (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=(CD105%20OR%20endoglin)+AND+micad%5Bbook%5D))
- Gene information in NCBI (CD105 (http://www.ncbi.nlm.nih.gov/gene/2022), TGF-β_1_ (http://www.ncbi.nlm.nih.gov/gene/7040))
- Articles in Online Mendelian Inheritance in Man (OMIM) (CD105 (http://www.ncbi.nlm.nih.gov/omim/131195), TGF-β_1_ (http://www.ncbi.nlm.nih.gov/gene/7040))
- Clinical trials (TRC105 (http://www.clinicaltrials.gov/ct2/results?term=TRC105))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=TRC105+AND+synthesis)]

DOTA-TRC105 was prepared as described previously (17). DOTA-TRC105 was purified with column chromatography. The number of DOTA moieties per mAb was not reported. DOTA-TRC105 (0.33 nmol) was incubated with 74 MBq (2 mCi) ^64^CuCl_2_ in sodium acetate buffer (pH 6.5) for 30 min at 40°C. ^64^Cu-DOTA-TRC105 was purified with column chromatography (16). This procedure provided a radiolabeling yield of >90%, with a specific activity of ~224 MBq/nmol (6.1 mCi/nmol) and a radiochemical purity of >98%. There were 0.42 ± 0.04 (n = 3) ^64^Cu ions per antibody molecule. ^64^Cu-DOTA-cetuximab was also prepared similarly as an isotype-matched control with similar specific activity. Cetuximab is an anti-EGFR mouse-human chimeric IgG_1_ mAb.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=TRC105+AND+in+vitro)]

Hong et al. (16) performed in vitro indirect fluorescence staining with the unlabeled TRC105 and DOTA-TRC105 on MCF7 human breast cancer cells (CD105-negative) and human umbilical vein endothelial cells (HUVECs, CD105-positive). Fluorescence microscopy and flow cytometry showed strong CD105 expression in HUVECs but weak or no expression in MCF7 cells. No significant differences in fluorescence intensities between TRC105 and DOTA-TRC105 were observed in the HUVEC cells, suggesting that DOTA-TRC105 retains immunoreactivity similar to that of the unconjugated mAb.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=TRC105+AND+in+vitro)]

Hong et al. (16) injected 5–10 MBq (0.14–0.27 mCi) ^64^Cu-DOTA-TRC105 into mice bearing the CD105-positive 4T1 murine breast tumors for ex vivo biodistribution and PET imaging studies (n = 3/group). Ex vivo tumor accumulation was 10% injected dose/gram (ID/g) and 7% ID/g at 24 h and 48 h after injection, respectively. The tumor/muscle ratios were 22.1 ± 1.5 and 25.2 ± 1.2 at 24 h and 48 h, respectively. The organ with the highest accumulation at 24 h was the liver (22% ID/g), followed by the spleen (12% ID/g), kidney (8% ID/g), and lung (4% ID/g). By 48 h, tumor accumulation was higher than that in all major organs. On the other hand, the accumulation of ^64^Cu-DOTA-cetuximab (control) in most organs was higher than that in the 4T1 tumors at 48 h after injection. The tumor accumulation of ^64^Cu-DOTA-cetuximab was ~35% of the accumulation of ^64^Cu-DOTA-TRC105 in the tumor (P < 0.05). Immunofluorescence staining of 4T1 tumor sections showed colocalization of CD31 with CD105 on the tumor endothelial cells (CD31- and CD105-positive) but not on tumor cells (CD31-negative, CD105-positive). On the other hand, there was only weak CD105 staining on the liver and spleen sections. The accumulation of ^64^Cu-DOTA-TRC105 in the 4T1 tumors was largely CD105 specific, whereas accumulation in the liver and spleen was largely CD105 nonspecific. Using the same tumor model, Yang et al. (18) reported that the circulation half-life of ^64^Cu-DOTA-TRC105 was 3.5 h and the circulation half-life of ^64^Cu-DOTA-cetuximab was 11.5 h.

PET imaging revealed estimated tumor accumulation of 8.0 ± 0.5% ID/g, 10.4 ± 2.8% ID/g, and 9.7 ± 1.8% ID/g at 4, 24, and 48 h after injection of ^64^Cu-DOTA-TRC105 (16), respectively. Accumulation in the liver was 26.6 ± 2.2% ID/g, 12.8 ± 0.7% ID/g, and 9.6 ± 0.6% ID/g at 4, 24, and 48 h, respectively. The radioactivity in the blood was 16.5 ± 1.3% ID/g, 8.0 ± 1.5% ID/g, and 6.5 ± 1.4% ID/g at 4, 24, and 48 h, respectively. The tumor accumulation of ^64^Cu-DOTA-cetuximab was <2.5% ID/g at 4, 24, and 48 h after injection. Injection of excess TRC105 (13 nmol) 2 h before ^64^Cu-DOTA-TRC105 inhibited tumor accumulation to the background level (<2% ID/g). The blocking effect of excess TRC105 on other organs was not reported.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=TRC105+AND+(dog+OR+rabbit+OR+pig+OR+sheep))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=TRC105+AND+(primate+NOT+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=TRC105+AND+human)]

No publication is currently available.

## References

1 Carmeliet P., Jain R.K. (2011). Molecular mechanisms and clinical applications of angiogenesis. Nature.
2 Folkman J. (1995). Angiogenesis in cancer, vascular, rheumatoid and other disease. Nat Med.
3 Fonsatti E., Altomonte M., Arslan P., Maio M. (2003). Endoglin (CD105): a target for anti-angiogenetic cancer therapy. Curr Drug Targets.
4 Abdollahi A., Folkman J. (2010). Evading tumor evasion: current concepts and perspectives of anti-angiogenic cancer therapy. Drug Resist Updat.
5 Thorpe P.E. (2004). Vascular targeting agents as cancer therapeutics. Clin Cancer Res.
6 Massague J., Cheifetz S., Laiho M., Ralph D.A., Weis F.M., Zentella A. (1992). Transforming growth factor-beta. Cancer Surv.
7 Cheifetz S., Bellon T., Cales C., Vera S., Bernabeu C., Massague J., Letarte M. (1992). Endoglin is a component of the transforming growth factor-beta receptor system in human endothelial cells. J Biol Chem.
8 Tabata M., Kondo M., Haruta Y., Seon B.K. (1999). Antiangiogenic radioimmunotherapy of human solid tumors in SCID mice using (125)I-labeled anti-endoglin monoclonal antibodies. Int J Cancer.
9 Bredow S., Lewin M., Hofmann B., Marecos E., Weissleder R. (2000). Imaging of tumour neovasculature by targeting the TGF-beta binding receptor endoglin. Eur J Cancer.
10 Wu A.M., Senter P.D. (2005). Arming antibodies: prospects and challenges for immunoconjugates. Nat Biotechnol.
11 Milenic D.E., Brechbiel M.W. (2004). Targeting of radio-isotopes for cancer therapy. Cancer Biol Ther.
12 Kowalsky, R.J., S.W. Falen, Radiopharmaceutcals in nuclear pharmacy and nuclear medicine. Second ed. 2004, Washington, D.C.: APhA. 733-752.
13 Seon B.K., Haba A., Matsuno F., Takahashi N., Tsujie M., She X., Harada N., Uneda S., Tsujie T., Toi H., Tsai H., Haruta Y. (2011). Endoglin-targeted cancer therapy. Curr Drug Deliv.
14 Fonsatti E., Jekunen A.P., Kairemo K.J., Coral S., Snellman M., Nicotra M.R., Natali P.G., Altomonte M., Maio M. (2000). Endoglin is a suitable target for efficient imaging of solid tumors: in vivo evidence in a canine mammary carcinoma model. Clin Cancer Res.
15 Tsujie M., Tsujie T., Toi H., Uneda S., Shiozaki K., Tsai H., Seon B.K. (2008). Anti-tumor activity of an anti-endoglin monoclonal antibody is enhanced in immunocompetent mice. Int J Cancer.
16 Hong H., Yang Y., Zhang Y., Engle J.W., Barnhart T.E., Nickles R.J., Leigh B.R., Cai W. (2011). Positron emission tomography imaging of CD105 expression during tumor angiogenesis. Eur J Nucl Med Mol Imaging.
17 Cai W., Chen K., He L., Cao Q., Koong A., Chen X. (2007). Quantitative PET of EGFR expression in xenograft-bearing mice using 64Cu-labeled cetuximab, a chimeric anti-EGFR monoclonal antibody. Eur J Nucl Med Mol Imaging.
18 Yang Y., Zhang Y., Hong H., Liu G., Leigh B.R., Cai W. (2011). In vivo near-infrared fluorescence imaging of CD105 expression during tumor angiogenesis. Eur J Nucl Med Mol Imaging.